# ^64^Cu-Labeled Oxo-DO3A-conjugated trastuzumab and PCTA-conjugated trastuzumab

Chemical name: | ^64^Cu-Labeled Oxo-DO3A-conjugated trastuzumab and PCTA-conjugated trastuzumab
Abbreviated name: | [^64^Cu]-Oxo-DO3A-trastuzumab and [^64^Cu]-PCTA-trastuzumab
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bifunctional%20chelating%20agents&cmd=DetailsSearch)]

A bifunctional chelating agent (BFC) such as 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) is often used to link a radionuclide with a monoclonal antibody (mAb) for the targeted imaging or radioimmunotherapy of cancers (1). However, a major limitation of using BFCs is that harsh reaction conditions such as high temperatures are required to facilitate the formation of the radionuclide-BFC complex (2). In addition, these complexes are not very stable in vivo. Ferreira et al. developed two BFCs, 1-oxa-4,7,10-triazacyclododecane-S-5-(4-nitrobenzyl)-4,7,10-triacetic acid (p-NO(2)-Bn-Oxo-DO3A) and 3,6,9,15-tetraazabicyclo[9.3.1]pentadeca-1(15),11,13-triene-S-4-(4-nitrobenzyl)-3,6,9-triacetic acid (p-NO(2)-Bn-PCTA), and showed that these chelators produced stable radiolabeled complexes with ^64^Cu under mild conditions ([^64^Cu]-Oxo-DO3A and [^64^Cu]-PCTA) (3). A preliminary ex vivo biodistribution study in mice showed that, compared with [^64^Cu]-DOTA, there was a lower accumulation of radioactivity in the liver with [^64^Cu]-Oxo-DO3A and [^64^Cu]-PCTA. It was also observed that clearance of the label from the kidneys of the animals was faster with [^64^Cu]-PCTA than with either [^64^Cu]-Oxo-DO3A or [^64^Cu]-DOTA (3).

Trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2) is a monoclonal antibody (mAb) that targets the HER2/neu receptor, which is overexpressed in several types of cancer and is indicative of a poor prognosis for the patient (4). This mAb was approved by the United States Food and Drug Administration for the treatment of various cancers, and its radiolabeled form has been evaluated for the detection and radioimmunotherapy of the disease (5). Because the characteristics and applications of trastuzumab are well understood, Ferreira et al. investigated and compared the in vitro and in vivo properties of the ^64^Cu-labeled PCTA, Oxo-DO3A, and DOTA conjugates of this mAb (2).

### Related Resource Links

EGFR- and HER2-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=EGFR+and+HER2+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=HER2) and protein (http://www.ncbi.nlm.nih.gov/protein?term=HER2) sequences of HER2

EGFR-related clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR) in ClinicalTrials.gov

HER2-related clinical trials (http://clinicaltrials.gov/ct2/results?term=human+epidermal+growth+factor+receptor+type+2+%28HER2%29) in ClinicalTrials.gov

Bioassays of EGFR (http://www.ncbi.nlm.nih.gov/pcassay?term=EGFR) and HER2 (http://www.ncbi.nlm.nih.gov/pcassay?term=HER2) in PubChem BioAssay

EGFR (http://omim.org/entry/131550) in Online Mendelian Inheritance in Man Database (OMIM)

Human EGFR signaling pathway (http://www.genome.jp/kegg-bin/show_pathway?hsa04012) in Kyoto Encyclopedia of genes and Genomes database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20synthesis&cmd=DetailsSearch)]

The synthesis of the PCTA-, Oxo-DO3A-, and DOTA-trastuzumab conjugates has been described by Ferreira et al. (2). The average numbers of chelate molecules per molecule of trastuzumab were 1.5 ± 0.4, 1.3 ± 0.2, and 1.7 ± 0.5 for Oxo-DO3A, PCTA, and DOTA, respectively, as determined with high-performance liquid chromatography (HPLC). The conjugates were labeled with ^64^Cu to obtain [^64^Cu]-PCTA-trastuzumab, [^64^Cu]-Oxo-DO3A-trastuzumab, and [^64^Cu]-DOTA-trastuzumab, and the radiochemical yields of the labeled bioconjugates (when 3.33 nmol of the conjugate was used in the labeling reaction) were >95%, >95%, and 88%, respectively (2). The final preparation of each radiolabeled mAb had a radiochemical purity of >95%. The specific activities of [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab were 0.36 ± 0.02 BGq/6.66 nmol (13.32 ± 0.74 mCi/6.66 nmol), 0.34 ± 0.01GBq/6.66 nmol (12.58 ± 0.37 mCi/6.66 nmol), and 0.24 ± 0.13 BGq/6.66 nmol (8.88 ± 4.81 mCi/6.66 nmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20in%20vitro%20studies&cmd=DetailsSearch)]

The stability of [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab was investigated by exposing the radiolabeled conjugates to mouse serum at 37°C for 24 h and 48 h (2). The amount of conjugate that remained intact after each time point was determined with HPLC analysis. After incubation for 24 h, both [^64^Cu]-PCTA- and [^64^Cu]-Oxo-DO3A-trastuzumab were >95% intact, but [^64^Cu]-DOTA-trastuzumab was only 54% intact at this time point. At 48 h, [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab were 80%, 78%, and 26% intact, respectively.

The receptor binding specificities of [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab were determined in a binding assay with SK-BR-3 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-30&Template=cellBiology) (these cells have a high expression of HER2 receptors (2 × 10^6^ receptors/cells)) (2). The binding values of [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab to the cells were 44 ± 5%, 33 ± 7%, and 33 ± 7% of the total radioactivity added in the assay, respectively. When the cells were exposed to excess nonlabeled trastuzumab (concentration not reported) prior to addition of the tracers, the binding of each radiolabeled bioconjugate was reduced to <2%. This indicated that the radiolabeled conjugates of trastuzumab had a high specificity of binding to HER2 expressed on the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab was studied in mice bearing HER2-positive (HER2^+^) and HER2-negative (HER2−) tumors (2). The HER2^+^ tumors were developed in the mice with LCC6^HER2^ cells, and the HER2− tumors were developed with LCC6^vector^ cells. The characteristics of the LCC6^HER2^ and the LCC6^vector^ cells are described by Dragowska et al. (6). The animals (n = 4 mice/radiolabeled trastuzumab conjugate) were given an intravenous injection of 5.5–7.4 MBq (203–278 μCi) [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, or [^64^Cu]-DOTA-trastuzumab, and whole-body positron emission tomographic (PET) images were acquired from the mice at 24 h and 40 h postinjection (p.i.). The rodents were euthanized at the end of each imaging session to harvest the organs of interest, including the tumors, to determine the amount of radioactivity accumulated in each organ. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). Although some differences were apparent with the three radiolabeled bioconjugates, in general they showed a similar background and biodistribution profile in the tissues of the animals (2). The uptake of radioactivity in the HER2^+^ tumors was significantly higher (P < 0.01) than that observed in the HER2− lesions. With each of these radiolabeled trastuzumab conjugates, the amount of tracer present in the blood, liver, kidneys, and the muscles was observed to decrease from 24 h p.i. to 40 h p.i. At 24 h p.i., a significantly higher uptake of radioactivity was observed in the HER2^+^ tumors with [^64^Cu]-PCTA- and [^64^Cu]-Oxo-DO3A-trastuzumab compared with [^64^Cu]-DOTA-trastuzumab (P = 0.014 and 0.006 for [^64^Cu]-PCTA- and [^64^Cu]-Oxo-DO3A-trastuzumab, respectively). In addition, at 24 h p.i. the tumor/kidney ratios for [^64^Cu]-PCTA- and [^64^Cu]-Oxo-DO3A-trastuzumab were >2-fold higher (P = 0.035) than with the ^64^Cu-labeled DOTA conjugate. The accumulation of ^64^Cu alone in the liver (20 ± 12% ID/g) and kidneys (7 ± 0.9% ID/g) was quite similar to that observed with the three radiolabeled biopharmaceuticals. This indicated that the three conjugates had a similar stability under in vivo conditions.

Whole-body PET images of the animals showed that, with all the radiolabeled conjugates, the radioactivity accumulated mainly in the HER^+^ tumors (2). A region of interest analysis of the tumors revealed that the ratios for the amount of radioactivity in the HER^+^ and the HER− tumors were 1.7, 2.3, and 1.4 at 24 h p.i. and 3.4, 2.8, and 3.7 at 40 h p.i. for [^64^Cu]-PCTA-, [^64^Cu]-Oxo-DO3A-, and [^64^Cu]-DOTA-trastuzumab, respectively.

From these studies, the investigators concluded that [^64^Cu]-PCTA- and [^64^Cu]-Oxo-DO3A-trastuzumab may be suitable for the early imaging of HER^+^ tumors in mice; however, it is necessary to confirm these observations with similar conjugates of other mAbs (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-Oxo-DO3A-trastuzumab%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Goldenberg D.M., Chang C.H., Rossi E.A. (2012). W. J, McBride, and R.M. Sharkey, Pretargeted molecular imaging and radioimmunotherapy. Theranostics.
2 Ferreira C.L., Yapp D.T., Crisp S., Sutherland B.W., Ng S.S., Gleave M., Bensimon C., Jurek P., Kiefer G.E. (2010). Comparison of bifunctional chelates for (64)Cu antibody imaging. Eur J Nucl Med Mol Imaging.
3 Ferreira C.L., Yapp D.T., Lamsa E., Gleave M., Bensimon C., Jurek P., Kiefer G.E. (2008). Evaluation of novel bifunctional chelates for the development of Cu-64-based radiopharmaceuticals. Nucl Med Biol.
4 Mitrasinovic P.M. (2012). Epidermal growth factor receptors: a functional perspective. Curr Radiopharm.
5 Carlsson J. (2012). Potential for clinical radionuclide-based imaging and therapy of common cancers expressing EGFR-family receptors. Tumour Biol.
6 Dragowska W.H., Warburton C., Yapp D.T., Minchinton A.I., Hu Y., Waterhouse D.N., Gelmon K., Skov K., Woo J., Masin D., Huxham L.A., Kyle A.H., Bally M.B. (2004). HER-2/neu overexpression increases the viable hypoxic cell population within solid tumors without causing changes in tumor vascularization. Mol Cancer Res.